# Anti-ICAM-1 antibody-conjugated paramagnetic liposomes

Chemical name: | Anti-ICAM-1 antibody-conjugated paramagnetic liposomes
Abbreviated name: | Anti-ICAM ACPLs
Synonym:
Agent category: | Antibody, small molecule (nanoparticle)
Target: | ICAM-1
Target category: | Antigen
Method of detection: | Magnetic resonance imaging (MRI), optical fluorescence microscopy
Source of signal/contrast: | Gadolinium, Texas Red
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=paramagnetic liposome ICAM)]

ICAM-1 (CD54) is a cell-surface glycoprotein belonging to the immunoglobulin superfamily of cell adhesion molecules (CAMs) (1). Upregulated by inflammatory mediators, ICAM-1 is expressed on various cells including leukocytes, epithelial cells, endothelial cells, and fibroblasts (2). The predominant function of ICAM-1 is the recruitment and trafficking of leukocytes through interactions with leukocyte-expressed integrins (2). Therefore, ICAM-1 plays a critical role in the development of the central nervous system (CNS), in immune and inflammatory responses, and in embryonic development (1). Many cerebrovascular and neurological diseases such as multiple sclerosis and its animal model (i.e., experimental allergic encephalomyelitis (EAE)), Alzheimer’s disease, and Parkinson’s disease have neuroinflammatory responses involving the migration of leukocytes into damaged or infected tissues (3). EAE, which is an ascending encephalomyelitis, is characterized by an intense perivascular inflammatory process in the white matter of the CNS, primarily on the spinal cord, brainstem, and cerebellum, which facilitates the attachment of leukocytes to inflamed endothelium (4). For example, a 10-fold increase in ICAM-1 expression has been found on the endothelium of capillaries and venules throughout the CNS at an early stage of EAE (4). Thus, ICAM-1 has been an attractive target for imaging the early and specific upregulation of vascular CAMs in diseases (4).

Amphiphiles are made from molecules containing both a hydrophobic (non-polar tail) and a hydrophilic (polar head) section. Amphiphiles can self-associate into multiple concentric lipid bilayers (called lamellae) in different sizes and geometries (5). Liposomes are generally formed by a variety of modified amphiphiles and can deliver a substantial amount of encapsulated therapeutic or diagnostic agents to targeted sites (6). Traditional liposomes suffer from the drawbacks of fast elimination from blood and easy capture by the reticulo-endothelial system (7). As an alternative to traditional liposomes, paramagnetic polymerized liposomes (PPLs) are composed of a mixture of lipids with different functional groups on the aqueous exposed surface and a polymerizable group (diacetylene) in the lipid tail (8). A typical formulation consists of gadolinium III–diethylenetriamine pentaacetic acid (Gd-DTPA)–based lipids, amphiphilic carrier lipids, and biotinylated amphiphiles (9).

PPLs possess increased physical stability, unique spectroscopic properties, and chemical modification durability (9). The diacetylene triple bonds in the PPLs are located in the fatty acyl chains. The polymerization of the triple bonds between lipids can be carried out by simple ultraviolet (UV) radiation to form a polydiacetylene backbone of alternating eneyne groups (8). A short polyethylene glycol (PEG) segment is covalently linked to the polar head of PPLs (9). The hydrophilicity of PEG allows for sterical stabilization of PPLs and protects against interactions with other molecular and biological components in blood stream, such as undesired lipid exchange or lipid fusion (9). Both polymerization and PEGylization prolong the in vivo circulation time of PPLs in blood. For instance, the half-life time of the PPLs is found to be ~19 h in rats (4). Because easy access to bulky water, the attachment of Gd-DTPA chelates on the surface of PPLs allows for greater relaxivity enhancement compared to Gd chelates entrapped in the traditional liposomes. The multiple Gd chelates on the surface of the liposomes further increase the sensitivity to detection by magnetic resonance imaging (MRI). The biotin groups in the PPLs allow for conjugation of biotinylated antibodies via an avidin-biotin linkage procedure (10). Avidin, a tetrameric protein with a molecular mass of 68 KDa, is capable of strongly binding four biotins (K_a_ = 1.7 × 10^15^ M^-1^) (10). Thus, avidins serve as a bridge between a biotinylated antibody against neural CAM (NCAM-1) and a biotinylated group on PPLs to form a NCAM-1–specific MRI contrast agent, anti-NCAM antibody-conjugated PPLs (ACPLs) (4).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(paramagnetic liposome ICAM)+AND+synthesis%0D%0A)]

Storrs et al. reported the details of synthesis of PPLs (9). Pentacosadiynoic acid (PDA) was treated with N-hydroxysuccinimide (NHS) and 1-(3-(dimethylamino)propyl)-3-ethylcarbodiimide hydrochloride (EDC) to form NHS ester, which was treated with a PEG-diamine linker (NH_2_(CH_2_CH_2_O)_2_CH_2_CH_2_NH_2_) to produce PEG-PDA derivatives. Then, the product was treated with DTPA dianhydride (DTPAA) to form DTPA-bis(PEG-PDA) diamides followed by a complexation with GdCl_3_ to produce a neutral amphiphilic Gd chelates. The PEG-PDA derivative was treated with biotinamidocaproic acid NHS ester to form biotinylated lipid conjugates. To generate PPLs, a mixture of 60% PEG-PDA, 29.5% Gd chelate lipid , 10% amino-terminated lipid, and 0.5% biotinylated lipid was polymerized at 0°C under irradiation from an ultraviolet lamp (wavelength = 254 nm) to form a dark blue PDA-PPLs. Sipkins et al. reported the details of preparation of anti–NCAM-1 ACPLs from the PPLs (4). ACPLs were formed by the addition of 2.3 μg avidin and 14.9 μg biotinylated antibody in a PPL solution at a concentration of 5.6 mM acyl chains.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( paramagnetic liposome ICAM)+AND+%22in+vitro%22)]

The T_1_ relaxivity of PPLs was determined to be 8.7 mM^-1^•s^-1^ at 2.0 T (8, 9). Gel electrophoresis and immunodetection techniques demonstrated the capability of attaching the monoclonal antibodies to biotinylated PPLs. The binding specificity of anti-ICAM-1 ACPLs was examined with an enzyme-linked immunosorbent assay (ELISA) in which the anti–ICAM-1 ACPLs competed with the inhibitory binding of horseradish peroxidase (HRP)-labeled anti–ICAM-1 antibodies (4). Then, the anti–ICAM-1 ACPL recognition of antigens was further confirmed in cultured endothelial cells with bacterial lipopolysaccharide–stimulated ICAM-1 expression. The multivalent anti–ICAM-1 ACPLs appeared to have significantly higher binding affinities compared to free antibody.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( paramagnetic liposome ICAM) +AND++rodentia)]

The in vivo targeting of anti–ICAM-1 ACPLs was examined in mice with EAE (4). Texas Red fluorophore-labeled anti-NCAM-1 ACPLs were administrated intravenously to EAE mice at 1.2 mg Gd/kg and 890 μg antibody/kg in the early phase of ICAM-1 upregulation. At 24 h after injection, brains were harvested for microscopic localization of fluorescent ACPLs. All EAE mice showed positive ACPL binding to CNS microvasculature in the cerebellum, brainstem, and spinal cord (4). The location of anti–ICAM-1 binding appeared to correlate with the immunohistochemically defined patterns for ICAM-1 expressions. For example, the binding of anti–ICAM-1 ACPLs was found in multiple vessels in the cerebellum that were surrounded by inflammatory infiltrates, in microvessels that were not associated with inflammatory infiltrates, and in small vessels but not in the large central arterioles. The complementary halves of the mouse brains were reserved from the fluorescence microscopy experiments and further imaged with high-resolution MRI microscopy techniques. Each brain was fixed in 45% paraformaldehyde, and T_1_-weighted images were collected on a 9.4 T imager. There were substantial increases in MRI signal intensity in the cerebellar (32%) and cerebral (28%) cortex, with moderate signal intensity increases in the cerebellar white matter (18%). The contrast between gray and white matter was improved particularly in the cerebellum because gray matter was significantly more vascularized than white matter. The PPLs had a blood plasma half-life of 19 h, which was comparable to that of PEG-stabilized liposomes (9).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( paramagnetic liposome ICAM) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( paramagnetic liposome ICAM) +AND+human)]

No publication is currently available.

### NIH Support

GM 07365

## References

1 Hubbard A.K., Rothlein R. (2000). Intercellular adhesion molecule-1 (ICAM-1) expression and cell signaling cascades. Free Radic Biol Med.
2 Hopkins A.M., Baird A.W., Nusrat A. (2004). ICAM-1: targeted docking for exogenous as well as endogenous ligands. Adv Drug Deliv Rev.
3 Turowski P., Adamson P., Greenwood J. (2005). Pharmacological targeting of ICAM-1 signaling in brain endothelial cells: potential for treating neuroinflammation. Cell Mol Neurobiol.
4 Sipkins D.A., Gijbels K., Tropper F.D., Bednarski M., Li K.C., Steinman L. (2000). ICAM-1 expression in autoimmune encephalitis visualized using magnetic resonance imaging. J Neuroimmunol.
5 Baxter A.G. (2007). The origin and application of experimental autoimmune encephalomyelitis. Nat Rev Immunol.
6 Strijkers G.J., Mulder W.J., van Heeswijk R.B., Frederik P.M., Bomans P., Magusin P.C., Nicolay K. (2005). Relaxivity of liposomal paramagnetic MRI contrast agents. Magma.
7 Torchilin V.P. (2005). Recent advances with liposomes as pharmaceutical carriers. Nat Rev Drug Discov.
8 Storrs R.W., Tropper F.D., Li H.Y., Song C.K., Sipkins D.A., Kuniyoshi J.K., Bednarski M.D., Strauss H.W., Li K.C. (1995). Paramagnetic polymerized liposomes as new recirculating MR contrast agents. J Magn Reson Imaging.
9 Storrs R.W., Tropper F.D., Li H.Y., Song C.K., Kuniyoshi J.K., Sipkins D.A., Li C.P.K., Bednarski M. (1995). Paramagnetic polymerized lyposomes: synthesis, characterization, and applications for magnetic resonance imaging. J. Am. Chem. Soc.
10 Mulder W.J., Strijkers G.J., Griffioen A.W., van Bloois L., Molema G., Storm G., Koning G.A., Nicolay K. (2004). A liposomal system for contrast-enhanced magnetic resonance imaging of molecular targets. Bioconjug Chem.